# N-[2-[4-(3-Cyanopyridin-2-yl)piperazin-1-yl]ethyl]-3-[^11^C]methoxybenzamide

Chemical name: | N-[2-[4-(3-Cyanopyridin-2-yl)piperazin-1-yl]ethyl]-3-[^11^C]methoxybenzamide
Abbreviated name: | [^11^C]7
Synonym:
Agent category: | Compound
Target: | Dopamine D_4_ receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20d4%20and%20carbon%20radioisotopes)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_-_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes have been classified into two subfamilies of D_1_-like (D_1_, D_5_) and D_2_-like (D_2_, D_3_, D_4_) dopamine receptors. D_1_-Like and D_2_-like receptors exert synergistic as well as opposite effects at the biochemical and overall system levels. A great majority of striatal D_1_ and D_2/3_ receptors are localized postsynaptically on the caudate-putamen neurons, and to a lesser extent presynaptically on nigrostriatal axons. On the other hand, D_4_ receptors are mostly found in the extrastriatal regions of the brain, such as the cortex, hippocampus, thalamus, and medulla. These areas are believed to control emotion and cognition.

In addition to D_2_ receptors, D_4_ receptors may play an important role in the pathophysiology of schizophrenia, as suggested by clinical studies of the atypical neuroleptic clozapine in patients (5, 6). Clozapine is not only effective against positive symptoms of schizophrenia, but it is also efficacious against the negative symptoms. Clozapine has a 10-fold greater affinity for D_4_ receptors than for D_2_ receptors (7). However, it also has high affinities for 5-HT_1A,1B,2A,2C,6,7_, α_1A,2A,2C_, muscarinic M_1_, and histamine H_1_ receptors. The neurophysiological role of D_4_ receptors remains to be defined. Thus, there is a need for selective ligands to investigate the pharmacological role of D_4_ receptors. There have been several attempts to develop specific D_4_ radioligands for use with positron emission tomography (PET) imaging of D_4_ receptors (8-10). However, none has proved suitable because of a lack of selectivity, extremely low D_4_ receptor density in the brain, and other pharmacological issues. Lacivita et al. (11) reported that N-[2-[4-(3-cyanopyridin-2-yl)piperazin-1-yl]ethyl]-3-methoxybenzamide (compound 7) is a potent inhibitor (agonist) of D_4_ receptors, with >100-fold selectivity over D_2_ and D_3_ receptors. This led to the development of N-[2-[4-(3-cyanopyridin-2-yl)piperazin-1-yl]ethyl]-3-[^11^C]methoxybenzamide ([^11^C]7) as a potential D_4_ receptor radioligand for use with PET imaging of D_4_ receptors in the brain.

### Related Resource Links:

- Chapters in MICAD (dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814), D_4_ receptor (http://www.ncbi.nlm.nih.gov/gene/1815))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451), D_4_ receptor (http://www.ncbi.nlm.nih.gov/omim/126452))
- Clinical trials (dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20d4%20and%20carbon%20radioisotopes%20AND%20synthesis%5bAll%20Fields%5d)]

Lacivita et al. (11) synthesized [^11^C]7 by reaction of [^11^C]CH_3_I with N-[2-[4-(3-cyanopyridin-2-yl)piperazin-1-yl]ethyl]-3-hydroxybenzamide for 3 min at 70°C. [^11^C]7 was purified with high-performance liquid chromatography (HPLC), with >99% radiochemical purity. The specific activity of [^11^C]7 was 2,770–3,890 GBq/μmol (74.9–105.1 Ci/µmol) at the end of synthesis. The radiochemical yield was 40.5 ± 10.8% (n = 4), with a total synthesis time of 28 min from the end of bombardment. The LogD_7.4_ value of compound 7 was 2.47.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20d4%20and%20carbon%20radioisotopes%20AND%20in%20vitro)]

Compound 7 was reported to have high binding affinities to D_4_ receptor sites but not to D_2/3_ receptors in recombinant HEK293 cell lines (11). The K_i_ value for D_4_ receptors using [^3^H]methylspiperone was 1.52 ± 0.20 nM. Compound 7 exhibited >100-fold selectivity over D_2_, D_3_, 5-HT_1A_, 5-HT_2A_, 5-HT_2C_, cannabinoid CB_1_, and sigma-1 receptors. Compound 7 exhibited D_4_ agonist activity by a decrease in forskolin-stimulated levels of cAMP accumulation in HEK293 cells expressing human recombinant D_4_ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_termDopamine%20d4%20and%20carbon%20radioisotopes%20AND%20rodentia)]

Lacivita et al. (11) performed ex vivo biodistribution studies in normal mice (n = 3) at 15, 30, 60, 120, and 240 min after intraperitoneal injection of 10 mg/kg unlabeled compound 7. Concentrations of compound 7 in the brain tissue and plasma were determined with HPLC. There was a rapid accumulation in the plasma, followed by a fast washout. The peak concentration in the plasma was 0.37 ± 0.21 µg/g at 30 min and became undetectable after 60 min. The concentration of an N-dealkylation metabolite, 1-(6-cyano-2-pyridyl)piperazine, was determined to be 0.22 ± 0.12 µg/g. The plasma concentrations of compound 7 and its metabolite at 30 min were 0.14 ± 0.02 µg/g and <0.1 µg/g, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20d4%20and%20carbon%20radioisotopes%20AND%20(dog%20or%20pig%20or%20rabbit%20ot%20sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20d4%20and%20carbon%20radioisotopes%20AND%20(primate%20not%20human))]

Lacivita et al. (11) performed dynamic PET brain scans on a male rhesus monkey for 90 min after injection of 38.5 MBq (1.04 mCi) [^11^C]7. The radioactivity accumulation in the hippocampus, striatum, cingulate cortex, entorhinal cortex, occipital cortex, and cerebellum peaked at 45 s and then declined. Little difference was observed between their time-radioactivity curves, suggesting no specific binding in these regions. About 3.1% injected dose reached the brain at 45 s. On the other hand, there was a gradual increase in radioactivity accumulation in the retina (reported to be rich in D_4_ receptors in rats) , which reached a plateau at 20–60 min. The retina/brain ratio was 6 at 90 min. No blocking studies were performed. The investigators concluded that a selective D_4_ ligand with higher affinity than compound 7 is needed for further studies.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20d4%20and%20carbon%20radioisotopes%20AND%20human)]

No publication is currently available.

## NIH Support

R01 MH063162, R01 MH063162-06S1

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Seeman P., Guan H.C., Van Tol H.H. (1993). Dopamine D4 receptors elevated in schizophrenia. Nature.
6 Seeman P., Guan H.C., Van Tol H.H., Niznik H.B. (1993). Low density of dopamine D4 receptors in Parkinson's, schizophrenia, and control brain striata. Synapse.
7 Van Tol H.H., Bunzow J.R., Guan H.C., Sunahara R.K., Seeman P., Niznik H.B., Civelli O. (1991). Cloning of the gene for a human dopamine D4 receptor with high affinity for the antipsychotic clozapine. Nature.
8 Bender D., Holschbach M., Stocklin G. (1994). Synthesis of n.c.a. carbon-11 labelled clozapine and its major metabolite clozapine-N-oxide and comparison of their biodistribution in mice. Nucl Med Biol.
9 Boy C., Klimke A., Holschbach M., Herzog H., Muhlensiepen H., Rota Kops E., Sonnenberg F., Gaebel W., Stocklin G., Markstein R., Muller-Gartner H.W. (1998). Imaging dopamine D4 receptors in the living primate brain: a positron emission tomography study using the novel D1/D4 antagonist [11C]SDZ GLC 756. Synapse.
10 Zhang M.R., Haradahira T., Maeda J., Okauchi T., Kawabe K., Noguchi J., Kida T., Suzuki K., Suhara T. (2002). Syntheses and pharmacological evaluation of two potent antagonists for dopamine D4 receptors: [11C]YM-50001 and N-[2-[4-(4-Chlorophenyl)-piperizin-1-yl]ethyl]-3-[11C]methoxybenzamide. Nucl Med Biol.
11 Lacivita E., De Giorgio P., Lee I.T., Rodeheaver S.I., Weiss B.A., Fracasso C., Caccia S., Berardi F., Perrone R., Zhang M.R., Maeda J., Higuchi M., Suhara T., Schetz J.A., Leopoldo M. (2010). Design, synthesis, radiolabeling, and in vivo evaluation of carbon-11 labeled N-[2-[4-(3-cyanopyridin-2-yl)piperazin-1-yl]ethyl]-3-methoxybenzamide, a potential positron emission tomography tracer for the dopamine D(4) receptors. J Med Chem.